# (R)-2-(N-Benzyl-4-(2-[^18^F]fluoroethoxy)phenylsulfonamido)-N-hydroxy-3-methylbutanamide

Chemical name: | (R)-2-(N-Benzyl-4-(2-[^18^F]fluoroethoxy)phenylsulfonamido)-N-hydroxy-3-methylbutanamide
Abbreviated name: | [^18^F]MMP-1f, [^18^F]1f
Synonym:
Agent Category: | Compound
Target: | Gelatinases (MMP-2 and MMP-9)
Target Category: | Enzyme binding
Method of detection: | PET
Source of signal/contrasat: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+1f)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of proteases are involved in atherogenesis, inflammation, myocardial infraction, angiogenesis, and tumor invasion and metastasis (4-8). The gelatinase family is a subgroup of MMPs consisting of gelatinase A (MMP-2) and gelatinase B (MMP-9) (9). Gelatinase expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of gelatinases have been found in tumors that are associated with a poor prognosis for cancer patients (10). A number of synthetic MMP inhibitors have been developed to block the activated MMPs in pathological conditions (11). (R)-2-(N-Benzyl-4-(2-fluoroethoxy)phenylsulfonamido)-N-hydroxy-3-methylbutanamide (1f) was found to be a potent MMP inhibitor (12). ^18^F-Labeled 1f ([^18^F]1f) is being developed for PET imaging of MMP proteolytic activity in tumors, atherosclerosis, myocardial infarction, and other diseases.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+1f+synthesis)]

[^18^F]1f was prepared as described by Wagner et al. (12). [^18^F]KF/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor, (R)-2-(N-benzyl-4-(2-(tosyloxy)ethoxy)phenylsulfonamido)-N-hydroxy-3-methylbutanamide, were heated in acetonitrile at 84°C for 4 min, followed by acidic hydrolysis in trifluoroacetic acid and high-performance liquid chromatography (HPLC). Average radiochemical yield was 12.4 ± 3.0% (n = 5) with a total synthesis time of 113 ± 6 min. Radiochemical purity was >97% with specific activities of 44 ± 19 GBq/µmol (1.19 ± 0.51 Ci/µmol) at end of synthesis. [^18^F]1f has a log D_7.4_ value of 2.02.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Wagner et al. (12) performed in vitro fluorogenic inhibition assays for MMP-2, MMP-8, MMP-9, and MMP-13. The MMP inhibitor 1f exhibited IC_50_ values of 4 ± 3 nM for MMP-2, 2 ± 1 nM for MMP-8, 50 ± 27 nM for MMP-9, and 11 ± 0.3 nM for MMP-13.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+1f+rodentia)]

Wagner et al. (12) performed biodistribution studies of [^18^F]1f in normal mice. [^18^F]1f accumulated mainly in the duodenum (uptake index (UI) = 10), kidney (UI = 5), and liver (UI = 2), with low blood, lung, heart, muscle, and brain radioactivity (UI < 0.3) at 20 min after injection. The UI for the tibia was about half that of the heart, indicating little defluorination of [^18^F]1f. Radioactivity levels in all tissues were very low by 60 min after injection with the exception of the bile (UI = 89 at 60 min). Approximately 53% of radioactivity in the plasma was intact [^18^F]1f at 20 min after injection with one polar metabolite as measured by HPLC. Pretreatment of 1f had little effect on the biodistribution and clearance of [^18^F]1f, indicating that there was little or no specific [^18^F]1f binding to MMPs in any of the normal tissues studied. The authors suggested that low accumulation of [^18^F]1f in normal tissues may be an advantage for future studies of activated MMPs in experimental animal models.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+1f+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed]

No publication is currently available.

## Human Studies

[PubMed]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix K., Dunkhorst A., Mayer K., Jordans S. (2007). and Cysteine cathepsins: Cellular roadmap to different functions. Biochimie.
8 Beaudeux J.L., Giral P., Bruckert E., Foglietti M.J., Chapman M.J. (2004). Matrix metalloproteinases, inflammation and atherosclerosis: therapeutic perspectives. Clin Chem Lab Med.
9 Nelson A.R., Fingleton B., Rothenberg M.L., Matrisian L.M. (2000). Matrix metalloproteinases: biologic activity and clinical implications. J Clin Oncol.
10 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
11 Skiles J.W., Gonnella N.C., Jeng A.Y. (2004). The design, structure, and clinical update of small molecular weight matrix metalloproteinase inhibitors. Curr Med Chem.
12 Wagner S., Breyholz H.J., Law M.P., Faust A., Holtke C., Schroer S., Haufe G., Levkau B., Schober O., Schafers M., Kopka K. (2007). Novel fluorinated derivatives of the broad-spectrum MMP inhibitors N-hydroxy-2(R)-[[(4-methoxyphenyl)sulfonyl](benzyl)- and (3-picolyl)-amino]-3-methyl-butanamide as potential tools for the molecular imaging of activated MMPs with PET. J Med Chem.